# ^99m^Tc-Anti-CD105 E9 monoclonal antibody

Chemical name: | ^99m^Tc-Anti-CD105 E9 monoclonal antibody
Abbreviated name: | ^99m^Tc-CD105 E9 MAb
Synonym: | ^99m^Tc-labeled- anti-endoglin MAb, ^99m^Tc-anti-endoglin MAb, ^99m^Tc-anti-EDG MAb, ^99m^Tc-anti-TGF-ß binding receptor MAb
Agent Category: | Antibody (Ab)
Target: | Endoglin (CD105, EDG)
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), Gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4557555), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=10862690) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2022) for more information about CD105

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD105+Mab)]

^99m^Tc-Anti-CD105 E9 monoclonal antibody (^99m^Tc-CD105 E9 MAb), which is formed by the ^99m^Tc conjugation of an intact E9 MAb against the antigen endoglin (cluster of differentiation 105 (CD105)), an accessory component of the receptor complex of transforming growth factor-β (TGF-β), has been developed for gamma imaging of tumor neovasculature (1). ^99m^Tc is a gamma emitter with a physical t_½_ of 6.01 h.

Because tumor growth and metastasis largely depend on angiogenesis, targeting of tumor vasculature is a promising strategy for cancer imaging and therapy (2). TGF-β is a pleiotropic cytokine that modulates angiogenesis, vascular remodeling, and tumor progression. Three isoforms of TGF-β, β_1_ to β_3_, have been identified. TGF-β_1_ appears to inhibit proliferation and migration of endothelial cells and their ability to form capillaries. CD105 (EDG) is a homodimeric cell membrane glycoprotein of 180 kDa, and it is a component of the TGF-β receptor complex that binds TGF-β_1_ and TGF-β_3_ with high affinity. CD105 is critical for correct blood vessel development. The expression of CD105 on different cells affects cellular response to TGF-β_1_. CD105 is overexpressed in proliferating endothelial cells of tumor vessels, and they prevent TGF-β_1_ inhibition of cellular proliferation (3, 4). Two isoforms of CD105, L and S, have been identified. L-CD105 is a protein of 633 amino acids and is expressed predominantly on endothelial cells. The molecular weight of CD105 is ~180,000 with disulfide-linked subunits of 95,000. The CD105 gene in humans has been mapped to chromosome 9q34→qter.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (5-7). Quiescent human endothelial cells express CD105 only weakly, but the expression of CD105 is strongly up-regulated on the endothelium of tumor tissues undergoing angiogenesis (4). The high level of expressed CD105 (up to 10^6^ molecules/proliferating cell) appears to be ideal for in vivo imaging and therapy. Tabata et al. (3) first investigated tumor targeting with ^125^I-labeled anti-CD105 MAbs in human breast tumor-bearing severe combined immune deficiency mice. The results showed the possible usefulness of antiangiogenic radioimmunotherapy with radiolabeled anti-CD105 MAbs. Anti-CD105 MAbs labeled with photon emitters can be used for tumor imaging. Fonsatti et al. (8) showed that a ^125^I-labeled anti-CD105 MAb (MAEND3) could efficiently image spontaneous mammary adenocarcinomas in two dogs. ^125^I is not an ideal radionuclide for imaging, but other radioactive iodines with better imaging properties are available. Alternatively, radiometals with appropriate gamma emissions, such as ^111^In and ^99m^Tc, are considered the radionuclides of choice for antibody imaging studies. The labeling with ^99m^Tc can generally be achieved by direct labeling without an additional chelating agent or indirect labeling with use of a bifunctional chelating agent (9, 10). In vitro Imaging of patient kidneys bearing tumors showed specific localization of ^99m^Tc-CD105 E9 MAb (1, 11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+cd105+mab)]

Costello et al. (1) developed a MAb, CD105 E9 (localized to chromosome 9q34), raised against CD105. CD105 E9 MAb was an IgG_1K_ with the number of sites for its binding = 1.1 × 10^5^/endothelial cell and K =2.91 × 10^11^ to CD105. CD105 E9 MAb was produced in mouse ascites and purified by affinity chromatography. Purified antibody fractions with concentration of 1 mg protein/ml in phosphate buffered saline were stored frozen until use. ^99m^Tc labeling was done with a reducing agent (stannous ion kit) in a direct labeling method. Five ml of CD105 E9 MAb (1 mg/ml) was added to 100 μl of stannous solution (from the methylene diphosphonate kit that contained stannous ions), after which 400 MBq (10.8 mCi) ^99m^Tc was added to the mixture for 10 min at room temperature. ^99m^Tc-CD105 E9 MAb was separated from unlabeled ^99m^Tc by use of a PD10 column. The labeling efficiency was 72-93%. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+cd105+mab)]

Costello et al. (1) studied localization of ^99m^Tc-CD105 E9 MAb in seven perfused kidneys with renal cell carcinomas obtained from patients. The solution of 50-200 MBq (1.35-5.4 mCi)/30 ml ^99m^Tc-CD105 E9 MAb was injected through the cannulated renal artery in vitro, and the kidney was allowed to incubate for up to 40 min at room temperature. The perfused kidney was then thoroughly washed with 200 ml of heparinized saline. In the immunoscintigraphy study (n = 7), well-defined hot spots of radioactivity were found in locations of tumor masses identified by preoperative magnetic resonance imaging scans as well as gross pathology studies. These hot spots were located mainly at the tumor periphery in the shape of a crescent. The radioactivity counts for all tumors were greater than those for the corresponding normal kidneys. ^99m^Tc counts in tumors were 4.1- to 113.0-fold (mean, 26.1-fold) higher than in normal kidneys. In two additional kidneys, blocking studies were performed by perfusing the kidneys first with unlabeled CD105 E9 MAb for 20 min before the injection of ^99m^Tc-CD105 E9. The results showed that the administration of unlabeled CD105 E9 MAb almost completely blocked the localization of ^99m^Tc-CD105 E9 MAb. In addition, immunofluorescence studies of the 7 studied kidneys showed that the endothelium lining of the microvessels in cryostat tumor sections had strong immunolocalization of CD105. However, the authors also reported that in a segment of microvessel, while most of the endothelial cells (ECs) were strongly positive for CD105, occasional ECs were negative. They suggested that the CD105-negative ECs were either mature ECs in the G_0_ phase of the cell cycle or apoptotic.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)+AND+in+vitro)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeled+CD105+MAb)++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeled+CD105+MAb)+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeled+CD105+MAb)+AND+human)]

No publication is currently available.

## References

1 Costello B., Li C., Duff S., Butterworth D., Khan A., Perkins M., Owens S., Al-Mowallad A.F., O'Dwyer S., Kumar S. (2004). Perfusion of 99Tcm-labeled CD105 Mab into kidneys from patients with renal carcinoma suggests that CD105 is a promising vascular target. Int J Cancer.
2 Fonsatti E., Altomonte M., Arslan P., Maio M. (2003). Endoglin (CD105): a target for anti-angiogenetic cancer therapy. Curr Drug Targets.
3 Tabata M., Kondo M., Haruta Y., Seon B.K. (1999). Antiangiogenic radioimmunotherapy of human solid tumors in SCID mice using (125)I-labeled anti-endoglin monoclonal antibodies. Int J Cancer.
4 Bredow S., Lewin M., Hofmann B., Marecos E., Weissleder R. (2000). Imaging of tumour neovasculature by targeting the TGF-beta binding receptor endoglin. Eur J Cancer.
5 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
6 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
7 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
8 Fonsatti E., Jekunen A.P., Kairemo K.J., Coral S., Snellman M., Nicotra M.R., Natali P.G., Altomonte M., Maio M. (2000). Endoglin is a suitable target for efficient imaging of solid tumors: in vivo evidence in a canine mammary carcinoma model. Clin Cancer Res.
9 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
10 Hnatowich D.J., Childs R.L., Lanteigne D., Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.
11 Duff S.E., Li C., Garland J.M., Kumar S. (2003). CD105 is important for angiogenesis: evidence and potential applications. Faseb J.